# ^111^In-Diethylenetriaminepentaacetic acid-aminohexanoic acid-Lys^40^-exendin-4

Chemical name: | ^111^In-Diethylenetriaminepentaacetic acid-aminohexanoic acid-Lys^40^-exendin-4
Abbreviated name: | ^111^In-DTPA-Ahx-Lys^40^-exendin-4
Synonym: | [Lys^40^(Ahx-DTPA-^111^In)NH_2_]exendin-4
Agent category: | Peptide
Target: | Glucagon-like peptide-1 (GLP-1) receptor
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=248418), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&val=1916066) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=14526) for more information about exendin-4.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-4)]

Glucagon-like peptide-1 (GLP-1, 30 amino acids) is secreted from enteroendocrine cells of the distal small intestine in response to food ingestion (1). It plays an important role in glucose metabolism and homeostasis. It inhibits gastric emptying, glucagon secretion, and glucose production (2). In addition, it induces insulin release from the pancreatic β-cells as well as their proliferation. The GLP-1 receptor has been identified in normal tissues such as the pancreas, stomach, brain, and lung, and it has been shown to be highly overexpressed in human insulinomas and gastrinomas (3). In insulinomas, GLP-1 receptor density is considerably greater and the GLP-1 receptor is more frequently observed than somatostatin receptors.

Exendin-4 is a GLP-1 analog with 39 amino acids isolated from the venom of the Gila monster (Heloderma suspectum) (4). Exendin-4 and GLP-1 share a 53% amino acid sequence homology. Exendin-4 is a more potent and longer-lasting GLP-1 receptor agonist than GLP-1. Exendin-4 is resistant to cleavage by dipeptidyl peptidase IV, whereas the first two N-terminal amino acids of GLP-1 are rapidly cleaved. Exenatide, a synthetic version of exendin-4, is the first GLP-1 mimetic recently approved by the US Food and Drug Administration (FDA) for use in select patients with type 2 diabetes (5). ^111^In-Diethylenetriaminepentaacetic acid-aminohexanoic acid-Lys^40^-exendin-4 (^111^In-DTPA-Ahx-Lys^40^-exendin-4) is being developed for single-photon emission computed tomography (SPECT) imaging of the GLP-1 receptor (6).

### Related Resource Links:

- Chapters in MICAD (GLP-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=GLP-1%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (GLP-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2740)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (GLP-1R (http://omim.org/entry/138032))
- Clinical trials (Exendin (http://www.clinicaltrials.gov/ct2/results?term=GLP-1))
- Drug information in FDA (Exendin (http://google2.fda.gov/search?q=exendin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-4%20and%20synthesis)]

A mixture of 100 MBq (2.7 mCi) ^111^InCl_3_ and diethylenetriaminepentaacetic acid-aminohexanoic acid-Lys^40^-exendin-4 (20 nmol) was incubated in sodium acetate buffer (pH 5.0) for 30 min at room temperature (6). ^111^In-DTPA-Ahx-Lys^40^-exendin-4 was identified with high-performance liquid chromatography and matrix-assisted laser desorption-ionization mass spectrometry (MALDI-MS) to have a radiochemical purity of >90%. The specific activity was 90 GBq/µmol (2.5 Ci/µmol). The labeling yield was >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-4%20and%20in%20vitro)]

Wild et al. (7) reported that ^111^In-DTPA-Ahx-Lys^40^-exendin-4 was 82% and 74% intact after 4.5 and 24 h of incubation in human serum at 37°C, respectively. DTPA-Ahx-Lys^40^-exendin-4 exhibited an inhibition constant (IC_50_) value of 2.1 ± 1.1 nM compared with 0.65 ± 0.1 nM for exendin-4 and 2.4 ± 0.1 nM for GLP-1 using ^125^I-labeled GLP-1 as a radioligand on mouse insulinoma β-cell tumors. ^111^In-DTPA-Ahx-Lys^40^-exendin-4 was specifically accumulated into β-cell tumors in culture with 2.4% of administered dose at 1 h and 9.8% at 4 h. Most of the accumulated radioactivity was internalized into the cells (85–97%).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-4%20and%20rodentia)]

Gotthardt et al. (6) performed biodistribution studies in normal mice and rats that consisted of injection of 1 MBq (37 μCi) ^111^In-DTPA-Ahx-Lys^40^-exendin-4. An experiment that consisted of coinjection of exendin-4 was also performed. Specific uptake was observed in the pancreas, stomach, lung, and spleen. Uptake in the kidneys and liver was not displaced by exendin-4. SPECT pinhole imaging in mice identified high uptake in the pituitary, lung, adrenals, and pancreas.

Wild et al. (7) extended the biodistribution studies by use of Rip1Tag2 mice with spontaneous insulinoma β-cell tumors. The organ with the highest uptake was the tumor [287% injected dose/g (% ID/g)], followed by kidneys (209% ID/g), lung (65% ID/g), pancreas (21% ID/g), stomach (5% ID/g), and liver (1% ID/g) at 4 h after injection of ^111^In-DTPA-Ahx-Lys^40^-exendin-4 (2 pmol/mouse). Excess unlabeled In-DTPA-Ahx-Lys^40^-exendin-4 blocked organ accumulation except in the kidneys. Blood clearance was fast, with 0.3% ID/g remaining in the blood 4 h after injection. In contrast, the tumor washout rate was slow. The tumor/blood ratio was 991 at 4 h and 2,200 at 48 h. SPECT pinhole imaging in mice identified high uptake in 5 small pancreatic tumors (1–3.2 mm) and kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-4%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-4%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-4%20and%20human)]

Christ et al. (8) performed whole-body SPECT scans in six patients with proven endogenous hyperinsulinemic hypoglycemia after injection of 90 MBq (2.4 mCi, 30 µg) of ^111^In-DTPA-Ahx-Lys^40^-exendin-4. The detection rate of insulinomas was 100% allowing successful surgical removal of the tumors in all patients.

## References

1 Theodorakis M.J., Carlson O., Michopoulos S., Doyle M.E., Juhaszova M., Petraki K., Egan J.M. (2006). Human duodenal enteroendocrine cells: source of both incretin peptides, GLP-1 and GIP. Am J Physiol Endocrinol Metab.
2 Doyle M.E., Egan J.M. (2001). Glucagon-like peptide-1. Recent Prog Horm Res.
3 Reubi J.C., Waser B. (2003). Concomitant expression of several peptide receptors in neuroendocrine tumours: molecular basis for in vivo multireceptor tumour targeting. Eur J Nucl Med Mol Imaging.
4 Meier J.J., Nauck M.A. (2005). Glucagon-like peptide 1(GLP-1) in biology and pathology. Diabetes Metab Res Rev.
5 Nielsen L.L., Young A.A., Parkes D.G. (2004). Pharmacology of exenatide (synthetic exendin-4): a potential therapeutic for improved glycemic control of type 2 diabetes. Regul Pept.
6 Gotthardt M., Lalyko G., van Eerd-Vismale J., Keil B., Schurrat T., Hower M., Laverman P., Behr T.M., Boerman O.C., Goke B., Behe M. (2006). A new technique for in vivo imaging of specific GLP-1 binding sites: First results in small rodents. Regul Pept.
7 Wild D., Behe M., Wicki A., Storch D., Waser B., Gotthardt M., Keil B., Christofori G., Reubi J.C., Macke H.R. (2006). [Lys40(Ahx-DTPA-111In)NH2]Exendin-4, a Very Promising Ligand for Glucagon-like Peptide-1 (GLP-1) Receptor Targeting. J Nucl Med.
8 Christ E., Wild D., Forrer F., Brandle M., Sahli R., Clerici T., Gloor B., Martius F., Maecke H., Reubi J.C. (2009). Glucagon-like peptide-1 receptor imaging for localization of insulinomas. J Clin Endocrinol Metab.